# Fluorescein-conjugated human serum albumin

Chemical name: | Fluorescein-conjugated human serum albumin
Abbreviated name: | FLS-HSA
Synonym:
Agent Category: | Human serum albumin
Target: | Non-target
Target Category: | Tumor infiltration
Method of detection: | Fluorescence
Source of signal: | Fluorescein
Activation: | Not required
Studies: | - Rodents | Fluorescein (FLS) linkage to human serum albumin (HSA)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorescein-human+serum+albumin+conjugate)]

Glioblastoma is a common and often lethal malignant form of brain cancer. Although there is a variety of treatments, such as chemotherapy, radiation, a combination of the two, and surgical resection, for patients with glioblastoma, the survival rate after treatment is <20% (1-3). This is primarily caused by recurrence of the disease as a result of incomplete surgical removal or exposure of the glioma tumors to radiation and chemotherapy during therapy. The difficulty in distinguishing the cancerous tissue from the normal surrounding tissue contributes to incomplete removal or treatment of the tumor. In addition, any surviving cancerous cells proliferate and tend to infiltrate other parts of the brain as a result of an inherent nature to migrate. Clear visualization of the tumor and its boundary would help in its complete removal or treatment and lead to improved prognosis for the patient.

Fluorescent dyes have been used for the visualization of glioma tumors, but the contrast between the tumor tissue and the normal tissue is not always clear, especially in the brain (4-6). Intravenous administration of fluorescein-sodium (FLS-Na) in human glioma patients has been used to visualize tumors, but a low contrast was observed between the cancerous tissue and normal tissue, which indicated that FLS-Na was not a very promising agent to visualize tumor boundary (6). Human serum albumin (HSA) can be used as a carrier for anti-cancer drugs and was shown to improve the circulating half-life of molecules conjugated to it (7, 8). In an effort to improve the fluorescence contrast, Ichioka et al. developed and evaluated a FLS-HSA conjugate for the visualization of tumors in a rodent model (3).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorescein-human+serum+albumin+conjugate+synthesis)]

The synthesis of FLS-HSA has been described by Ichioka et al. (3). For this, FLS-Na was dissolved in dimethylsulfoxide, and FLS was activated by dissolving dicyclohexylcarbodiimide and N-hydroxysuccinimide in this solution. This solution was left for 12 h at room temperature. Then HSA was dissolved in phosphate buffer (pH 7.4) and mixed with the activated FLS. The mixture was stirred for 30 min. The FLS-HSA conjugate was purified on a PD-10 column, and the eluted fractions that contained FLS-HSA were concentrated on an ApolloTM concentrator. The final concentration of HSA and FLS was adjusted to 10% and 0.2 mg/ml, respectively. The investigators did not provide data on the yield, purity, and FLS/HSA ratio of the preparation. As a control, FLS-Na was dissolved in lactate Ringer solution at a concentration of 0.2 mg/ml.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorescein-human+serum+albumin+conjugate+in+vitro)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The evaluation of FLS-HSA was performed with SCID (http://jaxmice.jax.org/library/notes/453a.html) mice bearing tumors generated with U251-MG cells, a human malignant glioma cell line (3). Either FLS-Na or FLS-HSA was administered intravenously through the tail vein. The animals were then sacrificed 15, 30, 60, 180, 360, and 720 min after the administration. The tumor nodules were exposed surgically and photographed with a digital camera attached to a fluorescence microscope. For reference, blood glucose analysis glassware filled with FLS-Na was prepared and placed near the tumor nodule when the photographs were taken. The brightness of the tumor nodule, normal tissue, and the reference standard was measured with Photoshop software. Three determinations were made and a mean, calibrated to the reference standard, was calculated. The contrast between the tumor nodule and normal tissue was determined and expressed as a tumor/peripheral brightness (t/p) ratio that was subjected to statistical analysis with ANOVA.

The t/p ratio was almost constant at 1.6 with FLS-Na between 15 and 180 min after administration. The fluorescence brightness diminished in both the tumor and the normal tissue 60 min after administration, and by 180 min the brightness was difficult to distinguish under the microscope. At this point the observations with FLS-Na were stopped. With FLS-HSA, the brightness was highest 15 min after administration of the reagent, but the t/p ratio of the tumor to normal tissue was >2.5 between 60 and 360 min after injection. The t/p ratios of FLS-HSA at 60, 180, and 360 min, and the peak t/p ratio of FLS-Na at 30 min, showed a significant statistical difference by ANOVA (P < 0.01). The investigators suggested that the low specificity shown by FLS-Na was probably because it can be passively transported and brightness can be observed at places where it may have accumulated as a result of unknown reasons. Intravenously administered HSA was shown to accumulate in tumor tissue (9), as observed in this study. Because HSA has a longer circulating half-life, a higher amount of FLS-HSA accumulated in the tumors and generated a brighter contrast compared to FLS-Na. The investigators concluded that although FLS-HSA has a distinct advantage over FLS-Na as a fluorescent tumor indicator, more work is required to determine its usefulness for human glioma surgery using an animal intracranial transplantation model. The investigators also mentioned that a limitation of this animal model was that the model lacked the blood–brain barrier present in the human brain as well as the infiltrating tumor cells of the human glioma that can exit into adjacent tissue of the patient’s brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorescein-human+serum+albumin+conjugate+Non-Primate+Mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorescein-human+serum+albumin+conjugate+Non-Human+Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No publications are currently available.

## References

1 Nakada M., Nakada S., Demuth T., Tran N.L., Hoelzinger D.B., Berens M.E. (2007). Molecular targets of glioma invasion. Cell Mol Life Sci.
2 Shrieve D.C., Alexander E., Black P.M., Wen P.Y., Fine H.A., Kooy H.M., Loeffler J.S. (1999). Treatment of patients with primary glioblastoma multiforme with standard postoperative radiotherapy and radiosurgical boost: prognostic factors and long-term outcome. J Neurosurg.
3 Ichioka T., Miyatake S., Asai N., Kajimoto Y., Nakagawa T., Hayashi H., Kuroiwa T. (2004). Enhanced detection of malignant glioma xenograft by fluorescein-human serum albumin conjugate. J Neurooncol.
4 Haglund M.M., Hochman D.W., Spence A.M., Berger M.S. (1994). Enhanced optical imaging of rat gliomas and tumor margins. Neurosurgery.
5 Poon W.S., Schomacker K.T., Deutsch T.F., Martuza R.L. (1992). Laser-induced fluorescence: experimental intraoperative delineation of tumor resection margins. J Neurosurg.
6 Kuroiwa T., Kajimoto Y., Ohta T. (1998). Development of a fluorescein operative microscope for use during malignant glioma surgery: a technical note and preliminary report. Surg Neurol.
7 Wunder A., Stehle G., Schrenk H.H., Hartung G., Heene D.L., Maier-Borst W., Sinn H. (1998). Antitumor activity of methotrexate-albumin conjugates in rats bearing a Walker-256 carcinoma. Int J Cancer.
8 Stehle G., Wunder A., Sinn H., Schrenk H.H., Schutt S., Frei E., Hartung G., Maier-Borst W., Heene D.L. (1997). Pharmacokinetics of methotrexate-albumin conjugates in tumor-bearing rats. Anticancer Drugs.
9 Leppala J., Kallio M., Nikula T., Nikkinen P., Liewendahl K., Jaaskelainen J., Savolainen S., Gylling H., Hiltunen J., Callaway J., et al. (1995). Accumulation of 99mTc-low-density lipoprotein in human malignant glioma. Br J Cancer.